# ^64^Cu-Labeled DOTA conjugated anti-epithelial membrane protein 2 minibody KS83

Chemical name: | ^64^Cu-Labeled DOTA-conjugated anti-epithelial membrane protein 2 minibody KS83
Abbreviated name: | [^64^Cu]-DOTA-KS83
Synonym:
Agent Category: | Antibody
Target: | Epithelial membrane protein 2
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=emp2%5bAll%20Fields%5d%20AND%20%28%22neoplasms%22%5bMeSH%20Terms%5d%20OR%20%22neoplasms%22%5bAll%20Fields%5d%20OR%20%22cancer%22%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

Endometrial membrane protein-2 (EMP2) is a member of the growth-arrest specific protein 3/peripheral myelin protein 22 family of proteins, which are believed to play a role in the development of endometrial cancer (http://cancer.gov/cancertopics/types/endometrial) in women (1). In addition, overexpression of EMP2 in endometrial cancer is considered to predict a negative outcome for the patient (2). Although the exact mechanisms of action of EMP2 are not known, it has been shown to modulate the translocation of molecules such as integrins, major histocompatibility complex-I, and glycophosphoinositol-linked proteins in the cell membrane (1). It has also been reported that EMP2 induces vascular endothelial growth factors in endometrial cancer tumors and promotes angiogenesis in lesions (3). In another study, it was shown that an engineered bivalent anti-EMP2 diabody suppressed the growth of HEC1A (human uterus/endometrium adenocarcinoma cell line) (4) and OVCARS5 (a human ovarian-endometrioid carcinoma cell line) (5) xenograft tumors in mice. Therefore, it was suggested that early detection and quantification of EMP2 could assist in the development of a suitable treatment regimen for patients suffering from endometrial cancer (6).

Fu et al. engineered an anti-EMP2 minibody (Mb, designated KS83; for a detailed structure of an Mb, see Fu et al. (6)), conjugated it to 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA), and labeled the conjugate with ^64^Cu, a positron emitter ([^64^Cu]-DOTA-KS83) (6). The non-radiolabeled Mb was investigated for its in vitro characteristics, and [^64^Cu]-DOTA-KS83 was evaluated with positron emission tomography (PET) for the detection of tumors that overexpressed EMP2 in mice (6).

### Related Resource Links

Minibody-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=minibody+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

EMP2 (http://www.ncbi.nlm.nih.gov/gene/2013) in Gene database (Gene ID: 2013)

Protein (http://www.ncbi.nlm.nih.gov/protein/4503561) and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/197304738) sequences of human EMP2

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Endometrial+cancer&Search=Search) on endometrial cancer

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20synthesis%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

The expression and purification of KS83 has been described elsewhere (6). The Mb was conjugated to DOTA and labeled with ^64^Cu as detailed by Fu et al. (6). Approximately 3 molecules of DOTA were determined to be linked with each molecule of KS83 (6). The labeling reaction was reported to have an efficiency of 97%, but the radiochemical yield (RCY) and radiochemical purity (RCP) of the labeled Mb were not reported (6). The specific activity (SA) of [^64^Cu]-DOTA-KS83 was 0.074 MBq/6.66 pmol (2 μCi/6.66 pmol).

For the biodistribution study, a ^64^Cu-labeled DOTA-anti CD20 Mb ([^64^Cu]-DOTA-CD20), an isotype Mb for the anti-EMP2 Mb, was used as a control (6). However, the RCY, RCP, and SA of the labeled Mb were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20vitro%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

Western blot analysis of different tissues from mice showed that EMP2 was present mainly in the lungs and vas deferens of the animals (6). Immunohistochemistry of the different tissues confirmed that EMP2 was expressed only in the epididymis and lungs of the mice; it was not detected in any other tissues of the animals (6). An analysis of human tissue arrays with anti-EMP2 sera revealed that the protein was expressed in the alveolar epithelium of the lungs, pigmented epithelium of the eye, the endometrium, and the epithelia of the vagina and the fallopian tubes (6). Immunohistochemical analysis of human tissues showed that EMP2 was expressed primarily in the lungs and endometrial tumors, but it was not detected in the spleen (6).

Flow cytometric analysis of DOTA-KS83 with HEC1A cells transfected at the EMP2 gene (HEC1A/EMP2 cells; these cells overexpress EMP2) showed that cellular binding of the DOTA-conjugated Mb (EC_50_ = 0.30 nM) was comparable to that of the purified KS83 (EC_50_ = 0.36 nM) (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20rodentia%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

The biodistribution of [^64^Cu]-DOTA-KS83 was investigated in mice bearing HEC1A/EMP2 cell tumors and wild-type HEC1A cell tumors (express normal amounts of EMP2) or Ramos cell tumors (negative controls; do not express EMP2) (6). The animals (n = 5 mice/time point) were injected with 0.074 MBq (2 μCi) labeled Mb through the tail vein, and PET images of the rodents were acquired at 4 h postinjection (p.i.) and at 20 h p.i. Control animals (n = 2 mice) were injected with [^64^Cu]-DOTA-CD20 and treated as described above. After the final imaging scan, the mice were euthanized and organs of interest were removed from the animals to determine the amount of radioactivity accumulated in the various tissues. Results obtained from this study were calculated as percent of injected dose per gram tissue (% ID/g) and are presented in Table 1. With [^64^Cu]-DOTA-KS83, maximum radioactivity was detected in the kidneys (36.4 ± 8.3% ID/g), followed by the liver (18.1 ± 1.6% ID/g) and the lungs (5.5 ± 1.1% ID/g) at 20 h p.i. All other organs showed an accumulation of <5% ID/g at 20 h p.i. At 4 h p.i., the HEC1A/EMP2 tumors showed an uptake of 7.3 ± 0.5% ID/g, which increased to 9.7 ± 1.9% ID/g at 20 h p.i. The wild-type HEC1A cell tumors showed an accumulation of 5.8 ± 0.8% ID/g at 4 h p.i., which decreased to 4.2 ± 1.3% ID/g at 20 p.i. The Ramos cell tumors accumulated only 2.3 ± 0.5% ID/g radioactivity at 20 h p.i. (the amount of label present in these tumors at 4 h p.i. was not determined). With [^64^Cu]-DOTA-KS83, 1.3-fold and 3-fold higher radioactivity accumulation was observed in the HEC1A/EMP2 tumors at 4 h p.i. and 20 h p.i., respectively, compared with [^64^Cu]-DOTA-CD20. No blocking studies were reported.

The PET images showed that the HEC1A/EMP2 cell tumors and the wild-type HEC1A cell tumors were clearly visible at 4 h p.i. and 20 h p.i., but the Ramos tumors (EMP2-negative) showed almost no uptake of radioactivity even at 20 h p.i (6). At 4 h p.i., the uptake of label was observed in the lung, heart, liver, and kidneys of all the animals, and a high amount of the label was detected in the liver and kidney even at 20 h p.i. No blocking studies were reported.

From these studies, the investigators concluded that [^64^Cu]-DOTA-KS83 is probably suitable for the detection and therapeutic monitoring of tumors that overexpress EMP2; however, more work is necessary before this ^64^Cu-labeled Mb can be used in the clinic (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20Other%5bAll%20Fields%5d%20AND%20Non-Primate%5bAll%20Fields%5d%20AND%20Mammals%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20Non-Human%5bAll%20Fields%5d%20AND%20Primates%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=64Cu%5bAll%20Fields%5d%20AND%20%28-anti-EMP2%5bAll%20Fields%5d%20AND%20minibody%5bAll%20Fields%5d%20AND%20Human%5bAll%20Fields%5d%20AND%20Studies%5bAll%20Fields%5d%29&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

These studies were supported by National Institutes of Health grants HD48540, R21 CA131756, CA016042, and R24 CA86307.

## References

1 Fu M., Rao R., Sudhakar D., Hogue C.P., Rutta Z., Morales S., Gordon L.K., Braun J., Goodglick L., Wadehra M. (2011). Epithelial membrane protein-2 promotes endometrial tumor formation through activation of FAK and Src. PLoS One.
2 Wadehra M., Natarajan S., Seligson D.B., Williams C.J., Hummer A.J., Hedvat C., Braun J., Soslow R.A. (2006). Expression of epithelial membrane protein-2 is associated with endometrial adenocarcinoma of unfavorable outcome. Cancer.
3 Gordon, L.K., M. Kiyohara, M. Fu, J. Braun, P. Dhawan, A. Chan, L. Goodglick, and M. Wadehra, EMP2 regulates angiogenesis in endometrial cancer cells through induction of VEGF. Oncogene, 2013
4 Shimazaki K., Lepin E.J., Wei B., Nagy A.K., Coulam C.P., Mareninov S., Fu M., Wu A.M., Marks J.D., Braun J., Gordon L.K., Wadehra M. (2008). Diabodies targeting epithelial membrane protein 2 reduce tumorigenicity of human endometrial cancer cell lines. Clin Cancer Res.
5 Fu M., Maresh E.L., Soslow R.A., Alavi M., Mah V., Zhou Q., Iasonos A., Goodglick L., Gordon L.K., Braun J., Wadehra M. (2010). Epithelial membrane protein-2 is a novel therapeutic target in ovarian cancer. Clin Cancer Res.
6 Fu M., Brewer S., Olafsen T., Wu A.M., Gordon L.K., Said J., Braun J., Wadehra M. (2013). Positron Emission Tomography Imaging of Endometrial Cancer Using Engineered Anti-EMP2 Antibody Fragments. Mol Imaging Biol.

Table 1: Uptake of radioactivity from [^64^Cu]-DOTA-KS83 and [^64^Cu]-DOTA-CD20 in various tissues of mice bearing HEC1A/EMP2 cell tumors, wild-type HEC1A cell tumors, or Ramos cell tumors.

Tissues | Uptake of radioactivity (% ID/g)
Tissues | 4 h p.i. | 20 h p.i.
HEC1A/EMP2 tumor | 7.3 ± 0.5 (6.1 ± 0.1) | 9.7 ± 1.9 (3.4 ± 0.6)
Wild type HEC1A tumor | 5.8 ± 0.8 (NA) | 4.2 ± 1.3 (NA)
Ramos tumor | ND (NA) | 2.3 ± 0.5 (NA)
Liver | 19.2 ± 5.4 (19.0 ± 3.1) | 18.1 ± 1.6 (26.6 ± 0.9)
Kidney | 47.1 ± 12.4 (33.1 ± 8.6) | 36.4 ± 8.3 (24.2 ± 8.2)
Lung | 12.5 ± 5.6 (12.1 ± 2.6) | 5.5 ± 1.1 (6.2 ± 0.9)
Heart | 9.2 ± 0.9 (8.3 ± 2.1) | 4.3 ± 1.0 (6.2 ± 0.7)
Blood | 18.1 ± 3.0 (13.2 ± 1.6) | 3.7 ± 0.6 (3.1 ± 1.9)
Uterus | 5.4 ± 0.8 (5.6 ± 2.7) | 4.9 ± 1.6 (4.9 ± 0.6)

Numbers in parenthesis represent the uptake of radioactivity in the tissue from [^64^Cu]-DOTA-CD20; NA: not available; ND: not determined. For complete data, see Fu et al. (6).